# ^111^In-Diethylenetriaminepentaacetic acid-2C5 monoclonal antibody

Chemical name: | ^111^In-Diethylenetriaminepentaacetic acid-2C5
Abbreviated name: | ^111^In-DTPA-2C5
Synonym:
Agent category: | Antibody
Target: | Nucleosome-specific antinuclear autoantibodies (ANA)
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography, gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%202C5)]

Natural autoantibodies are produced when the immune system recognizes one or more of the body's normal constituents as foreign. These autoantibodies attack the body's own cells, tissues, or organs, leading to systemic autoimmune diseases. Nucleosome-specific anti-nuclear autoantibodies (ANAs) have been found to exhibit anti-tumor activity (1). The nucleosomes targeted by these antibodies are released from the dying tumor cells and bind to the adjacent healthy tumor cells, leading to the formation of ANAs specific to the nucleosomes (2). The nucleosome-specific ANA monoclonal antibody (mAb) 2C5 was found to have anti-tumor activity against a variety of experimental tumor models but showed no recognition of normal cells (1). There was an increased survival rate in cancer patients with elevated levels of serum ANAs (3, 4). ^111^In-Diethylenetriaminepentaacetic acid-2C5 (^111^In-DTPA-2C5) has been studied for imaging ANA expression in nude mice bearing diverse human cancer xenografts (5, 6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%202C5+synthesis)]

Samokhin et al. (7) reported the radiolabeling of the mAb 2C5. DTPA-anhydride (0.5 mM) was added to a solution of the mAb 2C5 (~7 nmol) and dextran sulphate (MW, 10 kDa). The mixture was incubated for 1 h at room temperature. Excess DTPA was removed with dialysis. DTPA-2C5 was mixed with 1.11 MBq (0.03 mCi) ^111^InCl_3_ in citrate buffer (pH 3). The mixture was incubated for 60 min at room temperature. Excess ^111^In was removed from ^111^In-DTPA-2C5 with overnight dialysis. The ^111^In-labeling efficiency was 80% with a specific activity of 0.49 MBq/nmol (0.013 mCi/nmol). The radiochemical purity and the number of DTPA molecules per antibody were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%202C5+in+vitro)]

Chakilam et al. (5) showed that the binding affinity (K_d_) of 2C5 mAb for nucleosomes was 0.24 ± 0.06 nM. Flow cytometry analyses confirmed 2C5 mAb binding to eight broad variety human tumor cell lines (COLO-205, PC-3, C32TG, NCI-H82, MCF7, H9, H69 AR, and BT-20). DTPA-2C5 and 2C5 mAb exhibited similar immunoreactivity for immobilized nucleosomes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%202C5+rodentia)]

Chakilam et al. (5) performed biodistribution studies with ^111^In-DTPA-2C5 in mice bearing five broad variety human tumor xenografts (COLO-205, PC-3, C32TG, NCI-H82, and BT-20). The tumor/muscle ratios were 2.7–13.4 at 2 d after injection. Radioactivity levels in normal tissues/organs were not reported. Single-photon emission computed tomography scintigraphic imaging showed radioactivity as early as 6 h after injection and clearly visualized the radioactivity by 24 h, with high radioactivity in the abdomen area. Elbayoumi et al. (6) repeated the tumor accumulation study of ^111^In-DTPA-2C5 with two human tumor cell lines (COLO-205 and PC-3), which exhibited tumor/muscle ratios of 2.7 and 6.3 at 48 h, respectively. ^111^In-DTPA-2C5 liposomes exhibited tumor/muscle ratios of 6.0 for COLO-205 and 16.3 for PC-3 at 48 h, which were higher than the ratios obtained with ^111^In-DTPA-2C5 and ^111^In-labeled liposomes. High uptake of ^111^In-DTPA-2C5 liposomes was observed in the liver, spleen, and kidneys at just 3 h. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%202C5+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%202C5+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+2C5+human)]

No publication is currently available.

## NIH support

R01 EB01961, R01 EB02995, 2R01 HL55519

## References

1 Iakoubov L.Z., Torchilin V.P. (1997). A novel class of antitumor antibodies: nucleosome-restricted antinuclear autoantibodies (ANA) from healthy aged nonautoimmune mice. Oncol Res.
2 Iakoubov L.Z., Torchilin V.P. (1998). Nucleosome-releasing treatment makes surviving tumor cells better targets for nucleosome-specific anticancer antibodies. Cancer Detect Prev.
3 Blaes F., Klotz M., Huwer H., Straub U., Kalweit G., Schimrigk K., Schafers H.J. (2000). Antineural and antinuclear autoantibodies are of prognostic relevance in non-small cell lung cancer. Ann Thorac Surg.
4 Syrigos K.N., Charalambopoulos A., Pliarchopoulou K., Varsamidakis N., Machairas A., Mandrekas D. (2000). The prognostic significance of autoantibodies against dsDNA in patients with colorectal adenocarcinoma. Anticancer Res.
5 Chakilam A.R., Pabba S., Mongayt D., Iakoubov L.Z., Torchilin V.P. (2004). A single monoclonal antinuclear autoantibody with nucleosome-restricted specificity inhibits growth of diverse human tumors in nude mice. Cancer Therapy.
6 Elbayoumi T.A., Pabba S., Roby A., Torchilin V.P. (2007). Antinucleosome antibody-modified liposomes and lipid-core micelles for tumor-targeted delivery of therapeutic and diagnostic agents. J Liposome Res.
7 Samokhin G.P., Mongayt D.A., Iakoubov L.Z., Levchenko T.S., Torchilin V.P. (2001). Negatively charged polymers protect antinuclear antibody against inactivation by acylating agents. Anal Biochem.